# ^111^In-2-(4,7,10-Tris(carboxymethyl)-1,4,7,10-tetracyclododecan-1-yl)pentanedioic acid-Trastuzumab

Chemical name: | ^111^In-2-(4,7,10-Tris(carboxymethyl)-1,4,7,10-tetracyclododecan-1-yl)pentanedioic acid-Trastuzumab
Abbreviated name: | ^111^In-DOTAGA-Trastuzumab
Synonym:
Agent category: | Antibody
Target: | Epidermal growth factor receptor (EGFR, HER2)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Trastuzumab%20DOTAGA)]

Epidermal growth factor (EGF) is a growth factor composed of 53 amino acids (6.2 kDa), and it is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor patient prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, ^89^Zr-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-17). Moreau et al. (18) conjugated 2-(4,7,10-tris(carboxymethyl)-1,4,7,10-tetracyclododecan-1-yl)pentanedioic acid (DOTAGA), which is a derivative of 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA), to trastuzumab and labeled it with ^111^In as ^111^In-DOTAGA-trastuzumab for single-photon emission computed tomography (SPECT) imaging of HER2 expression in tumors.

### Related Resource Links:

- Chapters in MICAD (Trastuzumab (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Trastuzumab+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (EGF (http://www.ncbi.nlm.nih.gov/gene/1950), HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGF (http://omim.org/entry/131530), HER2 (http://omim.org/entry/164870))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), HER2 imaging (http://www.clinicaltrials.gov/ct2/results?term=HER2%20and%20imaging))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Trastuzumab%20DOTAGA%20and%20synthesis)]

Trastuzumab (20 nmol) was incubated with DOTAGA-anhydride (400 nmol) in phosphate-buffered saline (PBS) (pH, 7.4) for 30 min at 25°C (18). DOTAGA-Trastuzumab was isolated with ultrafiltration. There were 2.6 DOTAGA moieties per conjugate (148.9 kDa), as confirmed with mass spectroscopy_._ DOTAGA-Trastuzumab (0.83 nmol) was mixed with 125 MBq (3.4 mCi) ^111^InCl_3_ in ammonium acetate buffer (pH, 5.7) and incubated for 3 h at 37°C, with 66% labeling yield after removing free ^111^In^3+^ ions with ETDA treatment and isolation with ultrafiltration. The radiochemical purity was >97%. The specific activity was 150 MBq/nmol (4.1 mCi/nmol) at the end of synthesis. ^111^In-DOTAGA-Trastuzumab was >97% intact after incubation with 2,000-fold excess diethylenetriamine pentaacetic acid in PBS for up to 5 d.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Trastuzumab%20DOTAGA%20and%20in%20vitro)]

Moreau et al. (18) performed saturation binding experiments with ^111^In-DOTAGA-trastuzumab using the HER2-positive HCC1954 breast tumor cell line. The binding affinity (K_d_) value was 5.5 ± 0.6 nM. ^111^In-DOTAGA-Trastuzumab exhibited an immunoreactivity of 65%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Trastuzumab%20DOTAGA%20and%20rodentia)]

Moreau et al. (18) performed SPECT imaging scans in female nude mice (n = 4) bearing BT-474 human breast tumors at 24, 48, and 72 h after injection of 15 MBq (0.41 mCi) ^111^In-DOTAGA-trastuzumab (0.17 nmol). The tumors were clearly visualized at these time points. Region of interest analysis showed that the tumor accumulation of radioactivity was 11.0 ± 5.6% injected dose (ID), 13.1 ± 7.6% ID, and 14.0 ± 8.1% ID at 24, 48, and 72 h after injection, respectively. The radioactivity was located mainly in the rim of the tumor, with a lower radioactivity in the necrotic center of the tumor. The effective half-life (radioactive decay of ^111^In and biological excretion) of ^111^In-DOTAGA-trastuzumab in the mice was found with the image analysis to be 53.5 ± 4.0 h. The biological half-life (biological excretion) was calculated to be 268 ± 92 h. Ex vivo tissue biodistribution study was performed at 72 h after the last SPECT scan. Tumor accumulation was 66.9 ± 0.9% ID/g or 13.2 ± 8.2% ID. The highest radioactivity level was in the blood (10.0% ID/g), followed by the ovary (8.0% ID/g), spleen (6.9% ID/g), kidney (6.3% ID/g), lung (5.6% ID/g), liver (4.3% ID/g), heart (3.6% ID/g), and gastrointestinal tract (1.8% ID/g). Co-injection with 100-fold excess unlabeled trastuzumab reduced tumor accumulation by 73% at 72 h after injection, with little effect on the blood radioactivity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Trastuzumab%20DOTAGA%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Trastuzumab%20DOTAGA%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Trastuzumab%20DOTAGA%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Dijkers E.C., Oude Munnink T.H., Kosterink J.G., Brouwers A.H., Jager P.L., de Jong J.R., van Dongen G.A., Schroder C.P., Lub-de Hooge M.N., de Vries E.G. (2010). Biodistribution of 89Zr-trastuzumab and PET imaging of HER2-positive lesions in patients with metastatic breast cancer. Clin Pharmacol Ther.
18 Moreau, M., O. Raguin, J.M. Vrigneaud, B. Collin, C. Bernhard, X. Tizon, F. Boschetti, O. Duchamp, F. Brunotte, and F. Denat, DOTAGA-Trastuzumab. A New Antibody Conjugate Targeting HER2/Neu Antigen for Diagnostic Purposes. Bioconjug Chem, 2012